# 4,16α-[16α-^18^F]Difluoro-11β-methoxyestradiol

Chemical name: | 4,16α-[16α-^18^F]Difluoro-11β-methoxyestradiol
Abbreviated name: | 4F-M[^18^F]FES
Synonym:
Agent category: | Compound
Target: | Estrogen receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol))]

Estrogens and progestins are endogenous hormones that produce many physiological effects (1). Estrogens act primarily by regulating gene expression. Estrogen receptors (ERs) are found in the nucleus of cells of the female reproductive tract, breast, pituitary, hypothalamus, bone, liver, and other tissues, and also in various tissues in men. Estrogens are lipophilic in that they enter the cell passively by diffusion through the cellular membrane. They bind to ERs that are present in the nucleus.

Breast cancer is the most common malignancy in women. Approximately 33% of women who have this disease will die of disseminated breast cancer. The growth of breast epithelial cells is dependent on estrogen stimulation to induce progestin receptor expression. Two-thirds of breast carcinomas express ERs. It has also been established that the ER status of the tumor is an important prognostic indicator in breast cancer (2). Women with ER-positive breast tumors have a better prognosis than women with ER-negative tumors in terms of responsiveness to anti-estrogen treatment. ER content in breast cancer was assessed in vitro with receptor binding assays, which suffer from interassay variability and are also limited by intrinsic receptor heterogeneity of the tumor. 16α-[^18^F]Fluoro-17β-estradiol ([^18^F]FES) has been proven to be a valuable tracer for studies of the ER status of primary and metastatic breast cancer (3). However, [^18^F]FES is cleared from the blood and metabolized in 20 min with only 20% of [^18^F]FES intact in a study with 15 breast cancer patients (4). A newly developed estradiol analog, 4,16α-[16α-^18^F]difluoro-11β-methoxyestradiol (4F-M[^18^F]FES), exhibited favorable biodistribution in small animals and high uterus/background ratios in rodents (5) and humans (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol)%20AND%20synthesis)]

A one-pot automated synthesis of 4F-M[^18^F]FES was performed with the use of nucleophilic fluorination of the 3-methoxymethyl-4-fluoro-16β,17β-epiestriol-O-cyclic sulfone precursor (5). A solution of the precursor in acetonitrile was added to 2.2–3.0 GBq (60–80 mCi) [^18^F]fluoride and heated for 15 min at 110ºC. After removal of the solvent, a solution of ethanol and H_2_SO_4_ were added, and the mixture was heated at 110ºC for 10 min. 4F-M[^18^F]FES was isolated to provide radiochemical yields of 30–50% with a specific activity (decay-corrected) of ~111 GBq/µmol (~3 Ci/µmol) in ~120 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol)%20AND%20in%20vitro)]

ER binding affinity was assessed with competitive binding with [^3^H]estradiol in MCF-7 cells. The binding affinity of 4F-MFES was ~12% of estradiol (5). 4F-MFES showed little binding to human sex hormone-binding globulin and α-fetoprotein as compared with estradiol.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol)%20AND%20rodentia)]

It was demonstrated that 4F-M[^18^F]FES uptake by target tissue (uterus) in immature female rats (n = 8–10/group) is highly specific (5). Rats were injected with 1.85 MBq (0.05 mCi) 4F-M[^18^F]FES. The initial tracer accumulation in the uterus was 10.0 ± 1.8% injected dose per gram (ID/g) at 0.5 h, 14.7 ± 3.2% ID/g at 1 h, and 9.9 ± 1.8% ID/g at 4 h after injection. There was also a significant depression of 4F-M[^18^F]FES uptake (1.1 ± 0.3% ID/g) by the uterus at 1 h with co-injection of excess estrogen. The uptake in liver and kidneys was lower than uptake in the uterus. The accumulation of radioactivity in the bone was <0.25% ID/g. The uterus/blood ratios were 76, 136, and 109 at 0.5, 1, and 4 h after injection, respectively. [^18^F]FES exhibited the uterus/blood ratios of 27, 66, and 43 at 0.5, 1, and 4 h after injection, respectively. In general, 4F-M[^18^F]FES showed a higher accumulation than [^18^F]FES in the uterus but lower accumulation than [^18^F]FES in non-target tissues.

ER-positive murine mammary carcinomas MC7-L1 (19 ± 2 fmol/mg protein) and MC4-L2 (36 ± 12 fmol/mg protein) were compared for their accumulation of 4F-M[^18^F]FES and [^18^F]FES in female mice bearing the two tumors at 1 h after injection (7). The uptake values for the two tumors with 4F-M[^18^F]FES were 2.46% and 2.25% ID/g, which were lower than the uptake values of [^18^F]FES (3.12% ID/g and 3.42% ID/g). The uterus uptake values were 15.72% ID/g and 13.56% ID/g for 4F-M[^18^F]FES and [^18^F]FES, respectively. The tumor/blood ratios were 11.7 and 9.7 for 4F-M[^18^F]FES and [^18^F]FES, respectively. The uterus/blood ratios were 89.0 and 41.5 for 4F-M[^18^F]FES and [^18^F]FES, respectively. Co-injection of excess estradiol with 4F-M[^18^F]FES reduced the radioactivity levels in the tumors and uterus to the background level.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol)%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol)%20AND%20primates%20not%20humans)]

No relevant publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(4FMFES%20or%20difluoroestradiol)%20AND%20human)]

Human dosimetry of 4F-M[^18^F]FES was determined from blood samples and positron emission tomography images in 10 healthy women (age, 23–64 y) after intravenous injection of 66–201 MBq (1.8–5.4 mCi) 4F-M[^18^F]FES (6). The organ that received the highest absorbed dose was the gallbladder (0.80 mGy/MBq (3 rad/mCi)), followed by the upper large intestine (0.13 mGy/MBq (480 mrad/mCi)), small intestine (0.12 mGy/MBq (444 mrad/mCi)), and liver (0.10 mGy/MBq (370 mrad/mCi)). Uterus uptake was visualized in all subjects with a mean standardized uptake value of 2.68 ± 1.89 at 60 min after injection and an absorbed dose of 0.026 mGy/MBq (0.096 mrem/mCi). The effective dose equivalent was 0.026 mSv/MBq (96 mrem/mCi).

## References

1 Beato M., Klug J. (2000). Steroid hormone receptors: an update. Hum Reprod Update.
2 Vollenweider-Zerargui L., Barrelet L., Wong Y., Lemarchand-Beraud T., Gomez F. (1986). The predictive value of estrogen and progesterone receptors' concentrations on the clinical behavior of breast cancer in women. Clinical correlation on 547 patients. Cancer.
3 Flanagan F.L., Dehdashti F., Siegel B.A. (1998). PET in breast cancer. Semin Nucl Med.
4 Mankoff D.A., Tewson T.J., Eary J.F. (1997). Analysis of blood clearance and labeled metabolites for the estrogen receptor tracer [F-18]-16 alpha-fluoroestradiol (FES). Nucl Med Biol.
5 Seimbille Y., Rousseau J., Benard F., Morin C., Ali H., Avvakumov G., Hammond G.L., van Lier J.E. (2002). 18F-labeled difluoroestradiols: preparation and preclinical evaluation as estrogen receptor-binding radiopharmaceuticals. Steroids.
6 Beauregard J.M., Croteau E., Ahmed N., van Lier J.E., Benard F. (2009). Assessment of human biodistribution and dosimetry of 4-fluoro-11beta-methoxy-16alpha-18F-fluoroestradiol using serial whole-body PET/CT. J Nucl Med.
7 Benard, F., N. Ahmed, J.M. Beauregard, J. Rousseau, A. Aliaga, C. Dubuc, E. Croteau, and J.E. van Lier, [(18)F]Fluorinated estradiol derivatives for oestrogen receptor imaging: impact of substituents, formulation and specific activity on the biodistribution in breast tumour-bearing mice. Eur J Nucl Med Mol Imaging, 2008